# N-4-[^18^F]Fluorobut-2-yn-1-yl-2β-carbomethoxy-3β-phenyltropane

Chemical name: | N-4-[^18^F]Fluorobut-2-yn-1-yl-2β-carbomethoxy-3β-phenyltropane
Abbreviated name: | [^18^F]PR04.MZ
Synonym:
Agent category: | Compound
Target: | Dopamine transporter (DAT)
Target category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PR04.MZ)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion. Parkinson’s disease (PD) is associated with a loss of dopamine-containing neurons in the striatum, resulting in a loss of dopamine transporter (DAT) in the presynaptic nerve terminals (1, 2). Reduction of DAT density is inversely correlated with the severity of motor dysfunction in PD patients. Several (-)-cocaine analogs were developed for the evaluation of DAT density in neurons of PD patients. Radiolabeled 2β-carboxymethoxy-3β-(4-iodophenyl)tropane (β-CIT) and N-(3-fluoropropyl)-2β-carbomethoxy-3β-(4-iodophenyl)nortropane (FP-CIT) have been used for brain imaging (3-6). Because of the short physical half-life of ^11^C-labeled analogs, equilibrium conditions are difficult to achieve in positron emission tomography (PET) measurements. [^123^I]β-CIT was studied in single-photon emission computed tomography (SPECT) and showed slow tracer uptake kinetics (7, 8). A tropane derivative, [^11^C]-(E)-N-(4-fluorobut-2-enyl)-2β-carbomethoxy-3β-(4'-tolyl)nortropane ([^11^C]LBT-999), was evaluated as a radioligand for studies of DAT with PET imaging (9-11). N-4-[^18^F]Fluorobut-2-yn-1-yl-2β-carbomethoxy-3β-phenyltropane ([^18^F]PR04.MZ) was developed through the use of a conformational restriction approach based on (-)-cocaine (12). PR04.MZ exhibited a 100-fold higher potency than (-)-cocaine in inhibition of human DAT and better selectivity over the human noradrenalin transporter (hNET) and human serotonin transporter (hSERT). [^18^F]PR04.MZ has been evaluated as a radioligand for studies of DAT with PET imaging.

### Related Resource Links:

- Chapters in MICAD (DAT (http://www.ncbi.nlm.nih.gov/books?term=(DAT%20or%20dopamine%20transporter)%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (DAT (http://www.ncbi.nlm.nih.gov/gene/6531))
- Articles in Online Mendelian Inheritance in Man (OMIM) (DAT (http://www.ncbi.nlm.nih.gov/omim/126455))
- Clinical trials (DAT (http://www.clinicaltrials.gov/ct2/results?term=DAT+imaging))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PR04.MZ%20AND%20synthesis)]

[^18^F]PR04.MZ was readily synthesized by standard ^18^F-fluorination of the mesylate precursor with [^18^F]KF/Kryptofix 2.2.2 in acetonitrile for a few min at 120°C (12). [^18^F]PR04.MZ was purified with high-performance liquid chromatography. Overall radiochemical yield (non-decay corrected) was 13 ± 3%, with a specific activity of 18–95 GBq/µmol (0.5–2.6 Ci/µmol) at the end of synthesis and a radiochemical purity of >98%. Total synthesis time was 50 min.

## In Vitro studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PR04.MZ%20AND%20in%20vitro)]

PR04.MZ binding affinity for hDAT, hSERT, and hNET was determined using stably transfected HEK293 cells (12). [^3^H]β-CFT, [^3^H]citalopram, and [^3^H]nisoxetine were used as radioligands, respectively. The 50% inhibition concentration values for hDAT, hSERT, and hNET were 1.9 ± 0.2 nM, 108.4 ± 1.3 nM, and 22.5 ± 0.8 nM, respectively. In vitro autoradiography studies with [^18^F]PR04.MZ in rat brain sections showed a high radioactivity level in the striatum, with low binding in the cortical regions and cerebellum. Binding in the brain was totally blocked in the presence of 1 µM β-CFT.

## Animal Studies

### Rodents

[PubMed] (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PR04.MZ%20AND%20rodentia)

Riss et al. (12) performed ex vivo autoradiography studies in mouse brains (n = 3) after injection of 5 MBq (0.14 mCi) [^18^F]PR04.MZ at 35 min after injection. A high radioactivity level was observed in the striatum, with low binding in the cortical regions and cerebellum. The striatum/cerebellum ratio was 23.5. Binding in the striatum was totally blocked in the mice pretreated with 1.5 mg/kg β-CFT (n = 3 mice, 20 min before injection of [^18^F]PR04.MZ). Ex vivo biodistribution of [^18^F]PR04.MZ in normal rats (n = 3/group) was measured in the blood, brain, heart, liver, kidney, and bone at 5, 15, 30, and 60 min after injection. The initial standard uptake values (SUVs) at 5 min after injection were highest in the brain (7.0) and blood (7.3). The SUVs of both the brain and blood decreased to ~1.6 at 60 min. The liver (20.3), kidney (11.3), and heart (3.5) showed their highest SUVs at 15–30 min, with SUVs of 4.8, 3.8, and 1.2, respectively, at 60 min. The SUVs of bone were 0.2, 0.6, 1.5, and 1.5 at 5, 15, 30, and 60 min, respectively. [^18^F]PR04.MZ remained ~5% and ~94% intact in the plasma and brain, respectively, at 60 min.

Riss et al. (12) performed dynamic PR04.MZ PET brain scans in normal rats (n = 6). The peak striatal SUV of ~4 was reached at 20 min after injection with a striatum/cerebellum ratio of 7.3, which increased to 17.2 at 40 min. Injection of β-CFT (1.5 mg/kg) at 40 min after [^18^F]PR04.MZ reduced the striatum/cerebellum ratio to 5 at 20 min after β-CFT injection. β-CFT was able to displace [^18^F]PR04.MZ from binding to DAT.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PR04.MZ+AND+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PR04.MZ%20AND%20monkeys)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PR04.MZ%20AND%20human)]

No publication is currently available.

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Abi-Dargham A., Gandelman M.S., DeErausquin G.A., Zea-Ponce Y., Zoghbi S.S., Baldwin R.M., Laruelle M., Charney D.S., Hoffer P.B., Neumeyer J.L., Innis R.B. (1996). SPECT imaging of dopamine transporters in human brain with iodine-123-fluoroalkyl analogs of beta-CIT. J Nucl Med.
4 Chaly T., Dhawan V., Kazumata K., Antonini A., Margouleff C., Dahl J.R., Belakhlef A., Margouleff D., Yee A., Wang S., Tamagnan G., Neumeyer J.L., Eidelberg D. (1996). Radiosynthesis of [18F] N-3-fluoropropyl-2-beta-carbomethoxy-3-beta-(4-iodophenyl) nortropane and the first human study with positron emission tomography. Nucl Med Biol.
5 Kazumata K., Dhawan V., Chaly T., Antonini A., Margouleff C., Belakhlef A., Neumeyer J., Eidelberg D. (1998). Dopamine transporter imaging with fluorine-18-FPCIT and PET. J Nucl Med.
6 Lundkvist C., Halldin C., Ginovart N., Swahn C.G., Farde L. (1997). [18F] beta-CIT-FP is superior to [11C] beta-CIT-FP for quantitation of the dopamine transporter. Nucl Med Biol.
7 Ishikawa T., Dhawan V., Kazumata K., Chaly T., Mandel F., Neumeyer J., Margouleff C., Babchyck B., Zanzi I., Eidelberg D. (1996). Comparative nigrostriatal dopaminergic imaging with iodine-123-beta CIT-FP/SPECT and fluorine-18-FDOPA/PET. J Nucl Med.
8 Laruelle M., Wallace E., Seibyl J.P., Baldwin R.M., Zea-Ponce Y., Zoghbi S.S., Neumeyer J.L., Charney D.S., Hoffer P.B., Innis R.B. (1994). Graphical, kinetic, and equilibrium analyses of in vivo [123I] beta-CIT binding to dopamine transporters in healthy human subjects. J Cereb Blood Flow Metab.
9 Chalon S., Hall H., Saba W., Garreau L., Dolle F., Halldin C., Emond P., Bottlaender M., Deloye J.B., Helfenbein J., Madelmont J.C., Bodard S., Mincheva Z., Besnard J.C., Guilloteau D. (2006). Pharmacological characterization of (E)-N-(4-fluorobut-2-enyl)-2beta-carbomethoxy-3beta-(4'-tolyl)nortropane (LBT-999) as a highly promising fluorinated ligand for the dopamine transporter. J Pharmacol Exp Ther.
10 Dolle F., Emond P., Mavel S., Demphel S., Hinnen F., Mincheva Z., Saba W., Valette H., Chalon S., Halldin C., Helfenbein J., Legaillard J., Madelmont J.C., Deloye J.B., Bottlaender M., Guilloteau D. (2006). Synthesis, radiosynthesis and in vivo preliminary evaluation of [11C]LBT-999, a selective radioligand for the visualisation of the dopamine transporter with PET. Bioorg Med Chem.
11 Saba W., Valette H., Schollhorn-Peyronneau M.A., Coulon C., Ottaviani M., Chalon S., Dolle F., Emond P., Halldin C., Helfenbein J., Madelmont J.C., Deloye J.B., Guilloteau D., Bottlaender M. (2007). [11C]LBT-999: a suitable radioligand for investigation of extra-striatal dopamine transporter with PET. Synapse.
12 Riss P.J., Debus F., Hummerich R., Schmidt U., Schloss P., Lueddens H., Roesch F. (2009). Ex vivo and in vivo evaluation of [18F]PR04.MZ in rodents: a selective dopamine transporter imaging agent. ChemMedChem.